# ^131^I-Labeled recombinant anti-glycoprotein A33 antibody single chain variable fragment fused to cytosine deaminase

Chemical name: | ^131^I-Labeled recombinant anti-glycoprotein A33 antibody single chain variable fragment fused to cytosine deaminase
Abbreviated name: | [^131^I]A33scFv::CDy
Synonym:
Agent Category: | Antibody fusion protein
Target: | Glycoprotein A33
Target Category: | Antigen
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^131^I
Activation: | No
Studies: | - In vitro; - Rodents | Click here for protein and nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/50960640?ordinalpos=1&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) sequence of human glycoprotein A33.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=A33scFv%3A%3ACDy)]

The palmotylated glycoprotein A33 (gpA33) is a cell-surface differentiation antigen that belongs to the immunoglobulin superfamily (1, 2). This antigen is expressed primarily in the normal intestine and in >95% of colon tumors, and it has not been detected in any other tissue (1, 2). Because of its presence only in the intestine or in tumors in the intestine, the gpA33 has been evaluated as a target for the detection and radioimmunotherapy of colon cancer tumors (2). The biodistribution of a radioiodinated humanized monoclonal antibody (Ab) directed against the human gpA33 antigen (huA33) is discussed in a separate MICAD chapter (3). It was reported that the labeled Ab used to treat the colon cancers bound to the entire intestinal tissue, including the tumors; however, although the radioactivity persisted in the tumors for at least 6 weeks, the label was lost from the normal gut tissue within 1 week after administration (1-3). The more rapid clearance of a radioiodinated huA33 from the normal intestinal tissue was observed to correspond to the turnover period of basal colonocytes in this tissue (4).

Despite the extensive use of immunotherapy to treat cancers, the efficacy of this regimen is limited by the fact that not all individuals are responsive to this therapy. This is either due to the lack of or irresponsiveness of the receptors (or antigens) to which the Abs are directed. Also, because of its large size, the Ab may not be able to penetrate solid cancerous tumors completely, remain in blood circulation for extended periods, or may not be effective due to other factors as described by von Mehren et al. (5). As an alternative to Abs, investigators have developed Ab fragments such as the single chain variable fragments (scFv), which are much smaller (~30 kDa) than intact Abs (~150 kDa), contain the antigen-binding site, exhibit high tumor penetration, generate excellent tumor/normal tissue concentration ratios, and show rapid clearance through the kidneys (6, 7). Several scFv fragments targeted toward different antigens are under evaluation in clinical trials (http://clinicaltrials.gov/ct2/results?term=scFv) approved by the United States Food and Drug Administration and by similar regulatory agencies around the world (8).

To further enhance scFv efficacy for preclinical or clinical application, these protein chains have been linked, either by synthesis or recombinant methods, to a variety of molecules such as enzymes (for prodrug therapy), toxins (for treatment of cancer), etc., to generate bifunctional molecules (7, 9, 10). The scFv chain directs the enzyme or toxin to a predetermined cellular antigen where the enzyme converts a prodrug into a cytotoxic molecule or the toxin is activated and has a lethal effect on the cell. Therefore, an Ab fused to an enzyme could be used for an Ab-directed enzyme-prodrug therapy for the treatment of cancers or other diseases. On the basis of this principle, Coelho et al. fused a recombinant scFv directed against the A33 antigen (A33scFv) with the yeast cytosine deaminase (CDy) enzyme to generate A33scFv::CDy as a possible colon cancer treatment (6). The CDy part of the recombinant fusion protein deaminates 5-fluorocytosine (5-FC), the prodrug, to produce cytotoxic 5-fluorouracil after the A33scFv part binds to the A33 antigen on the cell surface. Therefore, the A33scFv::CDy fusion protein is selectively lethal to only those cells that overexpress the A33 antigen, i.e., colon cancer cells. Panjideh et al. investigated the binding specificity of ^131^I-labeled A33scFv::CDy under in vitro conditions and also studied its biodistribution in athymic mice bearing xenograft tumors derived either from LIM 1215 cells, a gpA33-positive human colon carcinoma cell line, or the negative control HT29 cells, a gpA33-negative human colon carcinoma cell line (11).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=A33scFv%3A%3ACDy+synthesis)]

The production and purification of A33scFv::CDy were described by Coelho et al. (6). Purity of the recombinant fusion protein was reported to be >95% as determined with sodium dodecylsulfate polyacrylamide gel electrophoresis. The ^131^I labeling of purified A33scFv::CDy, to obtain [^131^I]A33scFv::CDy, was done according to the chloramine-T method as detailed by Panjideh et al. (11). The specific activity of [^131^I]A33scFv::CDy was reported to be ~400 kBq/mg (~10.8 μCi/mg). The radiochemical yield, purity, and stability of the labeled fusion protein were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=A33scFv%3A%3ACDy131I+In+Vitro)]

The binding activity and specificity of A33scFv::CDy was investigated with the use of flow cytometry using LIM 1215 cells (6). Using a secondary polyclonal Ab directed toward the CDy part of the fusion protein, both the crude production supernatant and the purified fusion protein were shown to bind to the LIM 1215 cells. In another assay, the binding of A33scFv labeled with the green fluorescent protein (A33scFv::GF) to LIM 1215 cells was shown to be inhibited quantitatively by A33scFv::CDy, which suggested that the fusion protein bound specifically to the A33 antigen.

A cytotoxicity assay was performed to confirm the dual activity of A33scFv::CDy (6). LIM 1215 cells treated with A33scFv::CDy were exposed to different concentrations of 5-FC, and, with the use of appropriate controls, it was shown that 1 ng/ml of the fusion protein was sufficient for the maximum cytotoxic effect (25% cell survival) under these experimental conditions (6). Prior exposure of the cells to A33scFv::GF followed by treatment with A33scFv::CDy and 5-FC, as described above, was reported to eliminate the cytotoxic effects of the prodrug.

Using a saturation assay by exposing LIM 1215 cells to [^131^I] A33scFv::CDy, the equilibrium dissociation constant and the binding capacity of A33scFv::CDy were determined to be 15.8 nM and 5.02 nM/2 × 10^6^ cells, respectively (11).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=A33scFv%3A%3ACDy131I+Rodentia)]

To show the specificity of [^131^I]A33scFv::CDy binding to the A33 antigens in tumors, athymic mice (n = 4 animals/group) bearing either LIM 1215 cell (gpA33-positive) or HT29 cell (gpA33-negative) tumors were injected through the tail vein with the radiolabeled fusion protein (11). The animals were euthanized 47 h after treatment, and the tumors were removed to determine the amount of accumulated radioactivity. The LIM 1215 tumors were reported to accumulate ~90% of the injected dose/gram of tissue (% ID/g) compared with ~10% ID/g accumulated by the HT29 cell tumors. This indicated that the labeled fusion protein had a high binding specificity for cells expressing the A33 antigen.

The biodistribution of [^131^I]A33scFv::CDy was studied in athymic mice bearing LIM 1215 cell tumors (11). The animals were injected with [^131^I]A33scFv::CDy through the tail vein and euthanized at different time points (n = 4 animals/ time point) between 6 and 96 h after treatment. The various organs, including the tumors, were harvested and counted for accumulated radioactivity. By 47 h after injection the tumors were reported to accumulate almost 90% ID/g of the label, which decreased to ~20% ID/g by 96 h after treatment. In comparison, the other organs (liver, heart, and lungs) accumulated between ~2% ID/g and 10% ID/g during the entire period of the study. The kidneys were reported to accumulate between ~15% ID/g (at 67 and 96 h after treatment) and 70% ID/g (at 29 h after treatment), indicating that this was the label’s primary route of excretion.

In another study, mice bearing either LIM 1215 or HT29 cell xenograft tumors were treated with A33scFv::CDy followed by an injection of 5-FC 47 h later (11). The tumors were monitored daily, and by day 12 the LIM 1215 tumors were reported to shrink significantly (P = 0.0096) compared with the HT29 tumors, which were observed to have grown bigger during the observation period.

With results obtained from the various studies, the investigators concluded that A33scFv::CDy could probably be used for radioimmunotherapy, and its use for Ab-directed enzyme-prodrug therapy had therapeutic effects in a rodent model (11).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=A33scFv%3A%3ACDy131I+Non-Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=A33scFv%3A%3ACDy131I+Non-Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=A33scFv%3A%3ACDy131I+Human+Studies)]

No references are currently available.

## Supplemental Information

[Disclaimer]

No information is currently available.

## References

1 Sakamoto J., Kojima H., Kato J., Hamashima H., Suzuki H. (2000). Organ-specific expression of the intestinal epithelium-related antigen A33, a cell surface target for antibody-based imaging and treatment in gastrointestinal cancer. Cancer Chemother Pharmacol.
2 Ackerman M.E., Chalouni C., Schmidt M.M., Raman V.V., Ritter G., Old L.J., Mellman I., Wittrup K.D. (2008). A33 antigen displays persistent surface expression. Cancer Immunol Immunother.
3 Chopra, A., Radioiodinated humanized monoclonal antibody A33 [Radioiodinated-huA33 mAb]. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -2009.
4 Scott A.M., Lee F.T., Jones R., Hopkins W., MacGregor D., Cebon J.S., Hannah A., Chong G. (2005). P. U, A. Papenfuss, A. Rigopoulos, S. Sturrock, R. Murphy, V. Wirth, C. Murone, F.E. Smyth, S. Knight, S. Welt, G. Ritter, E. Richards, E.C. Nice, A.W. Burgess, and L.J. Old, A phase I trial of humanized monoclonal antibody A33 in patients with colorectal carcinoma: biodistribution, pharmacokinetics, and quantitative tumor uptake. Clin Cancer Res.
5 von Mehren M., Adams G.P., Weiner L.M. (2003). Monoclonal antibody therapy for cancer. Annu Rev Med.
6 Coelho V., Dernedde J., Petrausch U., Panjideh H., Fuchs H., Menzel C., Dubel S., Keilholz U., Thiel E., Deckert P.M. (2007). Design, construction, and in vitro analysis of A33scFv::CDy, a recombinant fusion protein for antibody-directed enzyme prodrug therapy in colon cancer. Int J Oncol.
7 Holliger P., Hudson P.J. (2005). Engineered antibody fragments and the rise of single domains. Nat Biotechnol.
8 Hudson P.J., Souriau C. (2003). Engineered antibodies. Nat Med.
9 Delves P.J., Roitt I.M. (2000). The immune system. First of two parts. N Engl J Med.
10 Delves P.J., Roitt I.M. (2000). The immune system. Second of two parts. N Engl J Med.
11 Panjideh H., Da Silva Coelho V.C., Dernedde J., Bachran C., Forster G.J., Franke J., Fasold P., Fuchs H., Thiel E., Deckert P.M. (2008). Biodistribution and efficacy of [131I]A33scFv::CDy, a recombinant antibody-enzyme protein for colon cancer. Int J Oncol.